# 2’-Fluoro-5-([^11^C]-methyl)-1-β-D-arabinofuranosyluracil

Chemical name: | 2’-Fluoro-5-([^11^C]-methyl)-1-β-D-arabinofuranosyluracil
Abbreviated name: | [^11^C]FMAU
Synonym:
Agent Category: | Compound
Target: | DNA
Target Category: | Incorporation into DNA
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FMAU&WebEnv=0cryXLMDpUTij6qeTX8ir6T87_vM-hfJEgkFrkaJGCLPtnlv2NCLI7UUC4kMNcr8qR4aHW1J-kAb_X%407748428072881B60_0000SID&WebEnvRq=1)]

Thymidine radiolabeled with radioactive C-14 or H-3 (TdR) is routinely used in vitro to measure cell proliferation and cell growth in various biological systems because it is a necessary and exclusive precursor for the synthesis of DNA (1). However, TdR can be easily catabolized by enzymes after in vivo administration and has resulted in the development of TdR derivatives that are not degraded and can be used to follow DNA synthesis to measure cell proliferation and growth (2, 3). Initially, a C- or H-labeled TdR was produced for imaging studies with positron emission tomography (PET); however, because this compound was catabolized and produced recirculating labeled products that reduced the tumor/normal tissue contrast, it was difficult to interpret results after its incorporation into DNA (4).

As a consequence, to circumvent the catabolite issue observed with TdR, some investigators developed TdR analogs that could be used for tumor imaging but were not catabolized (3, 5). Among the various TdR derivatives, those labeled with radioactive fluorine (^18^F) or ^11^C were developed to image and monitor tumors because, compared to normal tissue, rapid cell proliferation is a characteristic feature of these cancer lesions (6). Although [^18^F]-3’-deoxy-3’-fluorothymidine ([^18^F]FLT) has been used in the clinic to study different cancers, it has a limitation in that, within the cell, it is only converted into a triphosphate nucleoside, is not incorporated into the growing strand of DNA, and leads to DNA chain termination (7). The phosphorylation of FLT is taken to be an indicator of cytosolic thymidine kinase (TK_1_) activity rather than DNA synthesis, and the use of TK_1_ activity as a measure of DNA synthesis is not well established (8). Also, [^18^F]FLT is not a suitable agent to detect malignancies in the liver and bone marrow because it produces a high background in these tissue (9). In addition, because [^18^F]FLT is excreted through the urinary system, pelvic lesions may not be detected with this radiochemical (1).

Another analog of TdR, 1-(2’-deoxy-2’-fluoro-β-D-arabinofuranosyl)thymidine (FMAU) has been labeled with either ^18^F or ^11^C and used to study cell proliferation or image tumors in vivo (2, 10, 11). The only difference between FMAU and TdR is the substitution of a hydrogen atom with fluorine at the 2’-position of the deoxyarabinose sugar moiety in the molecule (2). FMAU was shown to possess the same biological properties as TdR, including transport across the cell membrane, enzymatic phosphorylation, and incorporation into cellular DNA (12). Compared to TdR, clearance of ^11^C-labeled FMAU ([^11^C]FMAU) from the blood was observed to be slower and showed a higher incorporation in tumors (12).

After conversion to a triphosphate, FMAU was shown to have an inhibitory effect on the hepatitis B virus polymerase and is approved by the United States Food and Drug Administration for evaluation in clinical trials (http://clinicaltrials.gov/ct2/results?term=FMAU) to treat this infection (13).

This chapter details the preclinical studies performed with [^11^C]FMAU. Studies performed with [^18^F]FMAU are presented in a separate chapter in MICAD (www.micad.nih.gov).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=11C+FMAU+synthesis&WebEnv=08kEtgGp2vRq8_r9anUrU4i5dx0P_HCTDZtJM8lcviaYL9MRzzk4KUGczlMgcm0acoPc_lr-asRFC0%407748428072881B60_0000SID&WebEnvRq=1)]

The synthesis of [^11^C]FMAU was described by Conti et al. (14). Initially, FMAU was prepared from 3’-5’-O-bis-(tetrahydropyranyl)-2’-fluoro-5-iodo-1-β-D-arabinofuranosyluracil (FMAU precursor). To obtain the FMAU precursor, 2’-fluoro-5-iodo-1-β-D-arabinofuranosyluracil (FIAU) was dissolved in dry tetrahydrofuran. p-Toluenesulfonic acid was added to this solution as a catalyst, followed by the addition of 2,3-dihydropyran. The mixture was stirred at room temperature for 2 h, and complete formation of the product was confirmed by thin-layer chromatography. The reaction was stopped with triethylamine. The solvent was subsequently evaporated, and the crude product was purified by preparative liquid chromatography on a silica gel column with acetone in hexane as an eluent. The solvent was evaporated to obtain the FMAU precursor as a white solid with a reaction yield of 93%.

For the synthesis of [^11^C]FMAU, the FMAU precursor was dissolved in dry tetrahydrofuranand cooled to -78°C, and n-butyllithium was added to it (14). Subsequently ^11^C-labeled methyl iodide was bubbled through the cold solution for 2 min, and then the reaction mixture was warmed to room temperature. After the addition of 2 M hydrochloric acid, the mixture was refluxed for 3 min in a heating block at 110°C. The residual solvent was then evaporated with argon, and the reaction was neutralized with 2 M sodium hydroxide after cooling. The crude product was separated by semipreparative high-performance liquid chromatography (HPLC), and purity of the product was checked by HPLC. On the basis of ^11^C-labeled methyl iodide, the product yield was 53% in 30–35 min from the end of bombardment. Radiochemical purity of [^11^C]FMAU was reported to be routinely >99% with a specific activity up to 100 Ci/mmol (3,700 Bq/mmol) (14). Stability of the product was not reported by the investigators (14).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=11C+FMAU+in+vitro&WebEnv=0NHuCzU_BZTwNqgCltjWTULC0v9Gmy-oeEKA4Fdjl_0JhWCIYahnicCAA9-8LNzGhe7fhJlOLg4ZLGl%407748428072881B60_0000SID&WebEnvRq=1)]

[^11^C]FMAU and [^18^F]-9-[(3-fluoro-1-hydroxy-2-propoxy)methyl]guanine ([^18^F]FHPG) incorporation into cellular DNA were evaluated to measure herpes simplex virus thymidine kinase (HSV-tk) enzyme activity after gene transfer into cells for the detection of human cytomegalovirus (HCMV) infections (15). Significantly higher amounts of both [^11^C]FMAU and [^18^F]FHPG were observed to accumulate in cells that express HSV-tk compared to the control cells. However, [^18^F]FHPG uptake in the cells that express HSV-tk was cell line–dependent, probably because the uptake depended either on the cell membrane transport characteristics or the cell enzyme substrate specificity. Both radiochemicals were reported to have a higher accumulation in HCMV-infected human umbilical vein endothelial cells compared to the uninfected control cells. A higher uptake of [^11^C]FMAU, compared to [^18^F]FHPG, was evident in the control cells and was postulated to be the result of host kinase phosphorylation activity (the subcellular identification of FMAU phosphates was not reported by the investigators). With results from this study, the investigators concluded that [^18^F]FHPG appeared to be more suitable than [^11^C]FMAU for prediction of HSV-tk gene therapy outcome and detection of HCMV infections with PET (15).

In another in vitro study, Davoodpour et al. determined that the incorporation of [^11^C]FMAU in prostate cancer cell aggregates was not a suitable marker to investigate the cytotoxicity of 2-methoxyestradiol, a metabolite of 17β-estradiol (16).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=11C+FMAU+rodentia&WebEnv=02ibe1u2ojtZnXsWKs-MB2qn35AAFB19k1O6gFe3V9-MeaI2Ak8V0IBWmZi5WWNcjW4zD0rG7sREOM4%407748428072881B60_0000SID&WebEnvRq=1)]

[^11^C]FMAU, [^18^F]FLT, and 1-(2'-deoxy-2'-fluoro-β-D-arabinofuranosyl)-5-[^76^Br]bromouracil ([^76^Br]BFU) were evaluated to determine tissue proliferation using DNA incorporation and excretion modulation as a readout in a rat model (3). Three groups (n = 4–7 animals per treatment group) of Sprague-Dawley rats were treated with the PET agents, and a subgroup of each treatment group was also administered cimetidine (a drug that was previously shown to increase the cellular DNA incorporation of [^76^Br]-BFU) to investigate whether it would increase the cellular incorporation of [^11^C]FMAU and [^18^F]FLT (17). The investigators observed that, among all the organs examined, organs with a high rate of DNA synthesis, i.e., the spleen and the intestines, had a maximum incorporation of the radiolabels (3). Although a gradual increase in [^76^Br]BFU in DNA was observed in the cimetidine-treated group, this drug did not affect the uptake of either [^11^C]FMAU or [^18^F]FLT. From these results the investigators concluded that, because [^76^Br]BFU was incorporated predominantly into the DNA, it could potentially be used as a PET agent for the measurement of in vivo cell proliferation. Similarly, [^11^C]FMAU could be used to determine cell proliferation, but, because its label had a short half-life, this radiochemical could not be used for an extended period of observation. They investigators also concluded that [^18^F]FLT was not suitable to measure cell proliferation because it was not incorporated into cellular DNA (3).

Bading et al. performed pharmacokinetic measurements with [^14^C]FMAU and PET studies with [^11^C]FMAU in rats bearing different types of syngeneic tumors (Dunning R3327-AT-2.1 and R3327-H prostate adenocarcinomas, and rat colorectal carcinomas) (12). With [^14^C]FMAU, the relative cell proliferation rates could be determined in normal tissue. FMAU was incorporated into the small intestine and colon tumor DNA. Among tumors, the highest uptake was observed in the rapidly growing colon carcinoma, but uptake was low in both the rapid- and the slow-growing prostate tumors. The investigators concluded that, although tumor uptake was modest and did not always correlate with the tumor growth rate, [^11^C]FMAU may be useful to image DNA synthesis in tissue (12).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=11C+FMAU+Non-Primate+Mammals&WebEnv=0SoUqK-GD_n1YsthgQETEu2v4gxBpADmvgmfGXMTwASstwFuNU9O6x5WtAylgUXk9-W218M-BiIKD--%407748428072881B60_0000SID&WebEnvRq=1)]

The uptake of [^11^C]FMAU was measured with PET in a canine brain tumor model (18). Dynamic imaging with arterial sampling was performed in beagle dogs (n = 8) that were administered [^11^C]FMAU after implantation of brain tumors. Six dogs were euthanized after a BUdR infusion and tumor time–activity curves (TACs) were obtained from computed tomography-defined regions of interest. The tumor volume occupied by viable cells was determined, and viable cells in the S-phase were identified by BUdR staining. Subsequently, a correlation between PET/[^11^C]FMAU and BUdR was determined. The tumor standardized uptake values (SUVs) and tumor/contralateral brain uptake ratios were respectively determined to be 1.6 ± 0.4 and 5.5 ± 1.2 at 50 min. No ^11^C-labeled metabolites of [^11^C]FMAU were observed in the blood up to 60 min after administration. The clearance of [^11^C]FMAU from plasma into the tumors correlated with the S-phase percent volume (P = 0.03), and the tumor SUV correlated significantly with both the S-phase and the cell percent volumes (P = 0.02 and 0.03, respectively). Tumor uptake and incorporation of [^11^C]FMAU was observed to correlate with the volume density of dividing cells (P = 0.0003) and not the nondividing cells (P = 0.3). From these observations the investigators concluded that the incorporation of [^11^C]FMAU correlated with tumor growth rate under the experimental conditions used for a canine brain tumor model, indicating that [^11^C]FMAU could be used to image cell proliferation in cancers (18).

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=11C+FMAU+nonhuman+primates&WebEnv=02ubWN5CSPt_UN3bmseaNq2zTspMfGA05w5VfPU4P2Ie7ZgDs1Hg9hhH1B8Zg-y1Q9Aiy5emkGmzrPg%407748428072881B60_0000SID&WebEnvRq=1)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=11C+FMAU+human+studies&WebEnv=0TeyRWMcrKyqNbn4HPanG5YSlx2rzwNZ0oM3bDNzTibg8t3XIw1ZsGGmmiMGCWgOM1esLCSfRaVAvzR%407748428072881B60_0000SID&WebEnvRq=1)]

No references are currently available.

## Supplemental Information

[Disclaimers]

## NIH Support

Some studies presented in this chapter were supported by the following grants: NIH grants CA-37870 and CA72896; NCI grants CA 72896, CA-18153, and CA-09022.

## References

1 Shields A.F. (2006). Positron emission tomography measurement of tumor metabolism and growth: its expanding role in oncology. Mol Imaging Biol.
2 Conti P.S., Hilton J., Wong D.F., Alauddin M.M., Dannals R.F., Ravert H.T., Wilson A.A., Anderson J.H. (1994). High performance liquid chromatography of carbon-11 labeled thymidine and its major catabolites for clinical PET studies. Nucl Med Biol.
3 Lu L., Samuelsson L., Bergstrom M., Sato K., Fasth K.J., Langstrom B. (2002). Rat studies comparing 11C-FMAU, 18F-FLT, and 76Br-BFU as proliferation markers. J Nucl Med.
4 Mankoff D.A., Shields A.F., Link J.M., Graham M.M., Muzi M., Peterson L.M., Eary J.F., Krohn K.A. (1999). Kinetic analysis of 2-[11C]thymidine PET imaging studies: validation studies. J Nucl Med.
5 Grierson J.R., Shields A.F., Zheng M., Kozawa S.M., Courter J.H. (1995). Radiosyntheses of labeled beta-pseudothymidine ([C-11]- and [H-3]methyl) and its biodistribution and metabolism in normal and tumored mice. Nucl Med Biol.
6 Krohn K.A., Mankoff D.A., Eary J.F. (2001). Imaging cellular proliferation as a measure of response to therapy. J Clin Pharmacol.
7 Reske S.N., Deisenhofer S. (2006). Is 3'-deoxy-3'-(18)F-fluorothymidine a better marker for tumour response than (18)F-fluorodeoxyglucose?. Eur J Nucl Med Mol Imaging.
8 Rasey J.S., Grierson J.R., Wiens L.W., Kolb P.D., Schwartz J.L. (2002). Validation of FLT uptake as a measure of thymidine kinase-1 activity in A549 carcinoma cells. J Nucl Med.
9 Groves A.M., Win T., Haim S.B., Ell P.J. (2007). Non-[18F]FDG PET in clinical oncology. Lancet Oncol.
10 Sun H., Sloan A., Mangner T.J., Vaishampayan U., Muzik O., Collins J.M., Douglas K., Shields A.F. (2005). Imaging DNA synthesis with [18F]FMAU and positron emission tomography in patients with cancer. Eur J Nucl Med Mol Imaging.
11 Tehrani O.S., Muzik O., Heilbrun L.K., Douglas K.A., Lawhorn-Crews J.M., Sun H., Mangner T.J., Shields A.F. (2007). Tumor imaging using 1-(2'-deoxy-2'-18F-fluoro-beta-D-arabinofuranosyl)thymine and PET. J Nucl Med.
12 Bading J.R., Shahinian A.H., Vail A., Bathija P., Koszalka G.W., Koda R.T., Alauddin M.M., Fissekis J.D., Conti P.S. (2004). Pharmacokinetics of the thymidine analog 2'-fluoro-5-methyl-1-beta-D-arabinofuranosyluracil (FMAU) in tumor-bearing rats. Nucl Med Biol.
13 Korba B.E., Furman P.A., Otto M.J. (2006). Clevudine: a potent inhibitor of hepatitis B virus in vitro and in vivo. Expert Rev Anti Infect Ther.
14 Conti P.S., Alauddin M.M., Fissekis J.R., Schmall B., Watanabe K.A. (1995). Synthesis of 2'-fluoro-5-[11C]-methyl-1-beta-D-arabinofuranosyluracil ([11C]-FMAU): a potential nucleoside analog for in vivo study of cellular proliferation with PET. Nucl Med Biol.
15 de Vries E.F., van Waarde A., Harmsen M.C., Mulder N.H., Vaalburg W., Hospers G.A. (2000). [(11)C]FMAU and [(18)F]FHPG as PET tracers for herpes simplex virus thymidine kinase enzyme activity and human cytomegalovirus infections. Nucl Med Biol.
16 Davoodpour P., Bergstrom M., Landstrom M. (2004). Effects of 2-methoxyestradiol on proliferation, apoptosis and PET-tracer uptake in human prostate cancer cell aggregates. Nucl Med Biol.
17 Lu L., Bergstrom M., Fasth K.J., Langstrom B. (2000). Synthesis of [76Br]bromofluorodeoxyuridine and its validation with regard to uptake, DNA incorporation, and excretion modulation in rats. J Nucl Med.
18 Conti P.S., Bading J.R., Mouton P.P., Links J.M., Alauddin M.M., Fissekis J.D., Ravert H.T., Hilton J., Wong D.F., Anderson J.H. (2008). In vivo measurement of cell proliferation in canine brain tumor using C-11-labeled FMAU and PET. Nucl Med Biol.